# ^68^Ga-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_

Chemical name: | ^68^Ga-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_
Abbreviated name: | ^68^Ga-DOTA-MG0
Synonym: | ^68^Ga-DOTA-minigastrin
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 receptor (CCK2R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gastrin+analogs)]

The gastrointestinal peptides gastrin and cholecystokinin-2 (CCK2) have various regulatory functions in the brain and gastrointestinal tract (1). Gastrin and CCK2 have the same COOH-terminal pentapeptide amide sequence, GWMDF-NH_2_, which is the biologically active site (2). Human gastrin is a peptide composed of 33 amino acids and also exists in several C-terminal–truncated forms (3). These truncated forms include minigastrin (MG0), which is a 13-residue peptide with the sequence of D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_. CCKs exist in a variety of biologically active molecular fragments that range from 4 to 18 amino acids and include sulphated and unsulphated CCK8, which is an octapeptide (DYMGWMDF-NH_2_) (4). Two CCK receptor subtypes have been identified in normal tissues by their binding affinities to gastrin. CCK1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK2 (CCK-B, brain) receptors have high affinity for gastrin (4). The sulphated CCK8 peptide displays high affinity for both CCK1 and CCK2 receptors, which are G-protein–coupled (5). These receptors have also been found to be overexpressed in a variety of tumor types (5). CCK2 receptors (CCK2R) have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (1). CCK1 receptors (CCK1R) have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas. Radiolabeled CCK8 peptides have been studied in tumors expressing CCK2Rs with good specificity for potential in vivo imaging.

Hellmich et al. (6) discovered a splice variant version (CCK2i4svR) of the CCK2R, which is expressed constitutively in human colorectal and pancreatic cancer (7, 8). MG0 was N-terminally conjugated with tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) for radiolabeling with ^111^InCl_3_ to form ^111^In-DOTA-MG0 for single-photon emission computed tomography (SPECT) imaging of tumors expressing CCK2R and CCK2i4svR (9). Brom et al. (10) have investigated the potential of ^68^Ga-DOTA-MG0 for positron emission tomography (PET) CCK2R-expressing tumors in nude mice.

### Related Resource Links:

- Chapters in MICAD (CCK2R (http://www.ncbi.nlm.nih.gov/books?term=cholecystokinin%20AND%20micad%5Bbook%5D%20AND%20table%5Btype%5D))
- Gene information in NCBI (CCK2R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CCK2R (http://omim.org/entry/118444))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin)]

MG0 was prepared with solid-phase peptide synthesis (10). The N-terminus was conjugated with a DOTA-chelating group to produce DOTA-MG0 by N-hydroxysuccinimidyl-DOTA. DOTA-MG0 was purified with reverse-phase high-performance liquid chromatography (HPLC). Radiolabeling was performed by mixing ^68^GaCl_3_ with DOTA-MG0 (6.2 nmol) at pH 3. The mixture was heated for 20 min at 95ºC. ^68^Ga-DOTA-MG0 was purified with HPLC. The radiochemical purity and specific activity were 99% and 30 GBq/µmol (0.81 Ci/µmol), respectively. The labeling yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin+and+in+vitro)]

Brom et al. (10) performed in vitro cell-based receptor-binding assays using ^111^In-DOTA-MG0 (5–10 pmol) on AR42J rat pancreatic tumor cells. The 50% inhibition concentration values were 2.4 nM, 3.2 nM, and 1.8 nM for DOTA-MG0, ^nat^In-DOTA-MG0, and ^nat^Ga-DOTA-MG0, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin+and+rodentia)]

Brom et al. (10) performed biodistribution studies of ^68^Ga-DOTA-MG0 in nude mice (n = 5) bearing subcutaneous AR42J tumors at 60 min after injection. Each mouse received 370 kBq (10 nCi) of ^68^Ga-DOTA-MG0 by intravenous injection. The tumor radioactivity level was 4.4 ± 1.3% injected dose per gram (ID/g). The uptake in the tumor was blocked by co-injection of excess DOTA-(His)_2_-minigastrin to 0.7 ± 0.1% ID/g. The kidney radioactivity level (90% ID/g) was not blocked by DOTA-(His)_2_-minigastrin. The blood, lung, stomach, intestines, pancreas, spleen, and liver radioactivity levels were <1% ID/g. The accumulation in the stomach (CCK2R rich) was almost completely blocked by DOTA-(His)_2_-minigastrin, whereas little blocking was observed in the other normal tissues. PET imaging showed that the tumors were clearly visualized at 60 min after injection of 5 MBq (0.14 mCi) ^68^Ga-DOTA-MG0 along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+minigastrin+and+human)]

No publication is currently available.

## NIH Support

1R01 AG030328-01

## References

1 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
2 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
3 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for peptide receptor-targeted radionuclide therapy. J Nucl Med.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Hellmich M.R., Rui X.L., Hellmich H.L., Fleming R.Y., Evers B.M., Townsend C.M. (2000). Human colorectal cancers express a constitutively active cholecystokinin-B/gastrin receptor that stimulates cell growth. J Biol Chem.
7 Smith J.P., Stock E.A., Wotring M.G., McLaughlin P.J., Zagon I.S. (1996). Characterization of the CCK-B/gastrin-like receptor in human colon cancer. Am J Physiol.
8 Smith J.P., Verderame M.F., McLaughlin P., Martenis M., Ballard E., Zagon I.S. (2002). Characterization of the CCK-C (cancer) receptor in human pancreatic cancer. Int J Mol Med.
9 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
10 Brom M., Joosten L., Laverman P., Oyen W.J., Behe M., Gotthardt M., Boerman O.C. (2011). Preclinical evaluation of 68Ga-DOTA-minigastrin for the detection of cholecystokinin-2/gastrin receptor-positive tumors. Mol Imaging.